# 4-[^18^F]Fluorobenzoyl-rhenium-cyclized-Ac-D-Lys-[Cys^3,4,10^, D-Phe^7^, Arg^11^]α-MSH_3-13_

Chemical name: | 4-[^18^F]Fluorobenzoyl-rhenium-cyclized-Ac-D-Lys-[ Cys^3,4,10^, D-Phe^7^, Arg^11^]α-MSH
Abbreviated name: | [^18^F]FB-RMSH
Synonym:
Agent category: | Peptide
Target: | Melanocortin-1 (MC-1) receptor, MC1R
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=27477129), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=27477128) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=4157&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about the Melanocortin-1 receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FB-RMSH)]

Malignant melanoma is the most deadly form of skin cancer (1). Early and accurate diagnosis is necessary for surgery and successful treatment (2). The melanocortin (MC) system is a neuropeptide network of the skin, and it is involved in pigmentation regulation, cortisol production, and many other physiological processes (3). Most cutaneous cell types express MC receptors, pro-opiomelanocortin (POMC), and prohormone convertases, and they also release MCs. Melanotropin-stimulating hormones (α-, β-, and γ-MSH) are derived from POMC by the proteolytic action of prohormone convertases. There are five MC receptors (MC1R to MC5R), which belong to the G-protein−coupled receptor superfamily. However, these receptors have been found to be overexpressed in melanoma cells (4, 5). α-MSH (Ac-Ser^1^-Tyr^2^-Ser^3^-Met^4^-Glu^5^-His^6^-Phe^7^-Arg^8^-Trp^9^-Gly^10^-Lys^11^-Pro^12^-Val^13^-NH_2_), produced by the brain and pituitary gland, is a tridecapeptide (13 amino acids) and is the most potent melanotropic peptide (6) in the regulation of skin pigmentation via MC1R.

Although positron emission tomography (PET) imaging with [^18^F]fluoro-2-deoxy-2-D-glucose ([^18^F]FDG) is effective in the detection of melanoma, it is not melanoma-specific and some melanoma cells do not take up [^18^F]FDG (7, 8). Radiolabeled α-MSH peptide analogs have been shown to specifically bind to MC1R that is overexpressed on human and mouse melanoma cells (4, 5, 7, 9, 10). Rhenium-cyclized α-MSH analogs have demonstrated high in vivo accumulation in tumors because of their high resistance to proteolysis (10, 11). A rhenium-cyclized α-MSH analog, Re-cyclized-Ac-D-Lys-[Cys^3,4,10^,D-Phe^7^,Arg^11^]α-MSH_3-13_ (RMSH), was radiolabeled with N-succinimidyl-4-[^18^F]fluorobenzoate ([^18^F]SFB) to form [^18^F]FB-RMSH as a potential positron emission tomography (PET) imaging agent to target melanoma (12).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Melanocortin-1%20+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (MC1R (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=4157))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=155555)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FB-RMSH+and+synthesis)]

Ren et al. (12) reported the synthesis of [^18^F]FB-RMSH. The Ac-D-Lys-[Arg^11^]α-MSH peptide was synthesized using standard Fmoc chemistry on an amide resin with a peptide synthesizer. Ac-D-Lys-[Arg^11^]α-MSH was then reacted with rhenium-glucoheptonate (1:1.5 molar ratio) for 30 min at 85°C. The cyclized peptide, RMSH, was purified with high-performance liquid chromatography (HPLC). HPLC analysis revealed two rhenium-cyclized isomers as RMSH-1 and RMSH-2, which were purified with HPLC and identified with mass spectroscopy. For ^18^F labeling, a solution of [^18^F]SFB and RMSH-1 or RMSH-2 peptide (100 ug) was heated for 60 min at 60°C. The maximum radiochemical yield was ~35% with a specific activity of 132-166 GBq/µmol (3.57-4.49 Ci/µmol) at the end of synthesis (decay-corrected). The radiochemical purities of [^18^F]FB-RMSH-1 and [^18^F]FB-RMSH-2 were >95% after HPLC purification. The total radiosynthesis time was ~ 3 h.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FB-RMSH+AND+in+vitro)]

Ren et al. (12) determined the 50% inhibition concentration (IC_50_) value of RMSH-1 and RMSH-2 to be 5.4 ± 0.7 and 13.9 ± 1.4 nM using B16/F1 murine melanoma cells with ^125^I-(Tyr^2^)-[Nle4, D-Phe]α-MSH (^125^I-NDP), respectively. In comparison, the IC_50_ values of FB-RMSH-1 and FB-RMSH-2 were 5.7 ± 0.7 and 9.0 ± 1.0 nM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FB-RMSH+AND+rodentia)]

Ren et al. (12) performed biodistribution studies in male C57BL/6 mice (n = 3/group) bearing B16/F1 murine melanoma tumors. Each mouse received 1.11 MBq (0.03 mCi) [^18^F]FB-RMSH-1. The tumor uptake radioactivity levels were obtained at 1 h, 2 h, and 4 h, respectively: 1.97 ± 0.39% injected dose per gram (% ID/g), 2.11 ± 0.12% ID/g, and 0.83 ± 0.05% ID/g. The tumor/blood and tumor/muscle ratios were 2.6 and 7.4 at 2 h after injection, respectively. Co-treatment with 9 nmol NDP reduced these ratios to 1.5 and 3.1 at 2 h after injection, respectively. The [^18^F]FB-RMSH-1 uptake in nontarget tissue (except the kidneys (5.4% ID/g), lung (2.4% ID/g) and liver (2.5% ID/g)) was low at 2 h. The radioactivity levels were 0.76% and 0.83% ID/g in the blood and bone at 2 h, respectively. The blood and bone radioactivity decreased to 0.39% and 0.30% ID/g at 4 h, respectively. [^18^F]FB-RMSH-2 exhibited similar biodistribution pattern except with higher kidney accumulation (16.9-17.8% ID/g) at 2 and 4 after injection.

PET imaging of mice bearing the B16F1 melanoma was conducted with intravenous injection of 13 MBq (0.35 mCi) [^18^F]FB-RMSH-1 or [^18^F]FB-RMSH-2 at 1 and 2 h after injection. The tumor, liver and kidneys were clearly visible. [^18^F]FB-RMSH-1 exhibited higher tumor accumulation but lower kidney accumulation than [^18^F]FB-RMSH-2.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FB-RMSH+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FB-RMSH+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FB-RMSH+AND+human)]

No publication is currently available.

## NIH Support

R24 CA93862, P50 CA114747

## References

1 Jemal A., Siegel R., Ward E., Murray T., Xu J., Thun M.J. (2007). Cancer statistics, 2007. CA Cancer J Clin.
2 Miao Y., Hylarides M., Fisher D.R., Shelton T., Moore H., Wester D.W., Fritzberg A.R., Winkelmann C.T., Hoffman T., Quinn T.P. (2005). Melanoma therapy via peptide-targeted {alpha}-radiation. Clin Cancer Res.
3 Bohm M., Luger T.A., Tobin D.J., Garcia-Borron J.C. (2006). Melanocortin receptor ligands: new horizons for skin biology and clinical dermatology. J Invest Dermatol.
4 Miao Y., Whitener D., Feng W., Owen N.K., Chen J., Quinn T.P. (2003). Evaluation of the human melanoma targeting properties of radiolabeled alpha-melanocyte stimulating hormone peptide analogues. Bioconjug Chem.
5 Siegrist W., Solca F., Stutz S., Giuffre L., Carrel S., Girard J., Eberle A.N. (1989). Characterization of receptors for alpha-melanocyte-stimulating hormone on human melanoma cells. Cancer Res.
6 Catania A., Airaghi L., Garofalo L., Cutuli M., Lipton J.M. (1998). The neuropeptide alpha-MSH in HIV infection and other disorders in humans. Ann N Y Acad Sci.
7 Weiner R.E., Thakur M.L. (2005). Radiolabeled peptides in oncology: role in diagnosis and treatment. BioDrugs.
8 Dimitrakopoulou-Strauss A., Strauss L.G., Burger C. (2001). Quantitative PET studies in pretreated melanoma patients: a comparison of 6-[18F]fluoro-L-dopa with 18F-FDG and (15)O-water using compartment and noncompartment analysis. J Nucl Med.
9 Tatro J.B., Reichlin S. (1987). Specific receptors for alpha-melanocyte-stimulating hormone are widely distributed in tissues of rodents. Endocrinology.
10 Chen J., Cheng Z., Owen N.K., Hoffman T.J., Miao Y., Jurisson S.S., Quinn T.P. (2001). Evaluation of an (111)In-DOTA-rhenium cyclized alpha-MSH analog: a novel cyclic-peptide analog with improved tumor-targeting properties. J Nucl Med.
11 Giblin M.F., Wang N., Hoffman T.J., Jurisson S.S., Quinn T.P. (1998). Design and characterization of alpha-melanotropin peptide analogs cyclized through rhenium and technetium metal coordination. Proc Natl Acad Sci U S A.
12 Ren G., Liu Z., Miao Z., Liu H., Subbarayan M., Chin F.T., Zhang L., Gambhir S.S., Cheng Z. (2009). PET of malignant melanoma using 18F-labeled metallopeptides. J Nucl Med.